# ^125^I-T84.66 scFv-human serum albumin

Chemical name: | ^125^I-T84.66 scFv-human serum albumin
Abbreviated name: | ^125^I-T84.66 scFv-HSA
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8).

Single-chain variable fragments (scFvs) of mAbs with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) and the minibody fragment (a dimer of scFvs-C_H_3 with a linker comprising 18 amino acids; molecular mass = 80 kDa) of a murine/human chimeric anti-CEA T84.66 antibody have been evaluated for targeting in several tumor antigen systems with rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 diabody and minbody, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. However, the pharmacokinetics of radiometal labeled antibodies, with high liver and kidney uptake, are generally not ideal for imaging (14). Albumin is known to accumulate in tumors (15) and has a long blood half-life (16). Furthermore, albumin fusion proteins have been shown to prolong the in vivo circulation of small peptides and proteins (17). A T84.66 single-chain antibody (scFv) was joined with human serum albumin (HSA) using recombinant technology to form T84.66 scFv-albumin fusion protein (T84.66 scFv-HSA), which was radiolabeled with ^125^I for localization of CEA-positive tumors in mice with single-photon emission computed tomography (SPECT) (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20+and%20synthesis)]

The recombinant T84.66 scFv-HSA (1.2 nmol) was labeled with 44.4 MBq (1.2 mCi) ^125^I in the presence of Iodogen at room temperature for 10 min (18). ^125^I-T84.66 scFv-HSA was isolated with size-exclusion chromatography with a radiolabeling efficiency of ~100%. The specific activity was ~37 MBq/nmol (1 mCi/nmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20+and%20in%20vitro)]

Radioimmunoreactivity of ^125^I-T84.66 scFv-HSA for recombinant CEA was determined to be 81% with high-performance liquid chromatography analysis (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20rodentia)]

Yazaki et al. (18) performed biodistribution studies of ^125^I-T84.66 scFv-HSA in nude mice (n = 5 mice/group) with the use of a LS174T human colon carcinoma subcutaneous xenograft model. Data were obtained at 0, 4, 18, 24, 48 and 72 h after injection. Accumulation of the ^125^I-T84.66 scFv-HSA in the CEA-expressing LS174T tumor was 12.3 ± 1.4% injected dose (ID)/g at 4 h and reached a maximum level of 22.7 ± 6.0% ID/g at 18 h. In comparison, ^125^I-T84.66 scFv and ^125^I-HSA reached a maximum of 4.9% ID/g at 0.5 h and 6% ID/g at 4 h, respectively. The liver, heart, spleen, lungs, and kidneys had lower levels of ^125^I-T84.66 scFv-HSA radioactivity than the LS174T tumor. The rapid blood clearance pattern exhibited a two-phase model with a half-life of 1 h during the distribution phase and a half-life of 15 h during the elimination phase. ^125^I-T84.66 scFv-HSA exhibited a markedly slower blood clearance than the T84.66 minibody and diabody but cleared faster than the parent T84.66 antibody. SPECT imaging with the ^125^I-T84.66 scFv-HSA showed high localization to the CEA-positive tumor and relatively low activity elsewhere (except the thyroid) in the mice, confirming the biodistribution data. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20human)]

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.
15 Wang J., Ueno H., Masuko T., Hashimoto Y. (1994). Binding of serum albumin on tumor cells and characterization of the albumin binding protein. J Biochem.
16 Dennis M.S., Zhang M., Meng Y.G., Kadkhodayan M., Kirchhofer D., Combs D., Damico L.A. (2002). Albumin binding as a general strategy for improving the pharmacokinetics of proteins. J Biol Chem.
17 Dennis M.S., Jin H., Dugger D., Yang R., McFarland L., Ogasawara A., Williams S., Cole M.J., Ross S., Schwall R. (2007). Imaging tumors with an albumin-binding Fab, a novel tumor-targeting agent. Cancer Res.
18 Yazaki P.J., Kassa T., Cheung C.W., Crow D.M., Sherman M.A., Bading J.R., Anderson A.L., Colcher D., Raubitschek A. (2008). Biodistribution and tumor imaging of an anti-CEA single-chain antibody-albumin fusion protein. Nucl Med Biol.